# [^124^I]Iodo-azomycin-galactoside

Chemical name: | [^124^I]Iodo-azomycin-galactoside
Abbreviated name: | [^124^I]IAZG
Synonym: | [^124^I]-1-(4-Deoxy-4-iodo-β-D-xylopyranosyl)-2-nitroimidazole
Agent Category: | Compound
Target: | Hypoxic cells
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IAZG)]

In a variety of solid tumors, hypoxia was found to lead to tumor progression and to resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy. It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized polarographic oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional, non-invasive imaging of intra-tumoral hypoxia has been demonstrated to be a feasible measurement of tumor oxygenation (7). This has led to the search and development of hypoxia-targeted, non-invasive markers of tumor hypoxia.

Chapman proposed the use of 2-nitroimidazole compounds for hypoxia imaging (8). 2-Nitroimidazole compounds are postulated to undergo reduction in hypoxic condition, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). [^18^F]Fluoromisonidazole [^18^F]FMISO) is the most widely used positron emission tomography (PET) tracer for imaging tumor hypoxia (7). However, [^18^F]FMISO has slow clearance kinetics and a high lipophilicity, resulting in substantially high background in PET scans. Novel 2-nitroimidazole compounds, such as [^18^F]FETA, [^18^F]FETNIM, 4-Br[^18^F]FPN, [^18^F]EF1, and [^18^F]EF5, are currently being investigated as potential markers of tumor hypoxia [PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=nitroimidazole+and+imaging)]. [^124^I]Iodo-azomycin-galactoside ([^124^I]IAZG) is a second-generation hypoxic marker of iodinated azomycin nucleosides with greater water solubility than other 2-nitroimidazole compounds, which increases renal excretion (10). [^124^I]IAZG is being evaluated as a PET probe for the detection of tumor hypoxia.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IAZG+synthesis)]

Schneider et al. (11) reported that [^125^I]IAZG was synthesized by exchange reaction between IAZG and ^125^I-NaI with 60% radiochemical yield. [^125^I]IAZG had a specific activity of 10.2 GBq/mmol (276 mCi/mmol). Zanzonico et al. (12) produced [^124^I]IAZG from IAZG and ^124^I-NaI with a radiochemical purity of >98%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IAZG+in+vitro)]

[^125^I]IAZG (10 μM) accumulated in EMT-6 tumor cells at a rate of 13.6 pmol/10^6^ cells per h (10). High oxygen concentration decreased and low oxygen concentration increased the rate of accumulation. No blocking studies were performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IAZG+rodentia)]

Schneider et al. (11) performed biodistribution studies of [^125^I]IAZG in mice bearing EMT-6 tumors. The biodistribution was fast except in the brain, where it was significantly lower, and in the liver and the kidney, where it was significantly higher. The tracer was rapidly cleared from the blood (plasma half-life, 0.46 h) with rapid renal and hepatobillary clearance within 2–3 h. There was a relative accumulation of the tracer in tumor with time (tumor/muscle and tumor/blood ratios were 23.0 and 9.9, respectively, at 6 h after injection). The maximal tumor uptake was at 0.5 h with 3.27 ± 0.08% injected dose (ID)/g. The liver (0.77 ± 0.22% ID/g) and kidney (0.79 ± 0.16% ID/g) exhibited lower accumulation than the tumor (1.54 ± 0.19% ID/g) at 2 h. No blocking studies were performed.

Zanzonico et al. (12) performed serial microPET imaging to evaluate [^124^I]IAZG as a hypoxia imaging agent in 17 MCa breast tumors and 6 FSaII fibrosarcomas implanted in mice. For comparison, [^18^F]FMISO was also imaged in the same tumor-bearing animals. Twelve animals were also imaged with [^18^F]fluorodeoxyglucose ([^18^F]FDG). Both [^124^I]IAZG and [^18^F]FMISO images showed high tracer uptake in the large tumors (>300 mg, pO_2_ < 2.5 mmHg in 67% of tumors). In [^18^F]FMISO images at 1, 3–4, and 6–8 h after injection, there was considerable whole-body background radioactivity. In contrast, [^124^I]IAZG imaging was optimal when performed at 24–48 h with low whole-body background. As a result, the [^124^I]IAZG images at 24–48 h had higher tumor/whole body activity contrast than the [^18^F]FMISO images at 3–6 h. A tumor uptake of 5–10% (of total body radioactivity) was visualized for [^18^F]FMISO at 3–6 h; tumor uptake for [^124^I]IAZG at 48 h was ~17%. Furthermore, biodistribution data showed that the tumor/normal tissue ratios (normal tissue includes the blood, heart, lung, liver, spleen, kidney, intestine, and muscle) of [^124^I]IAZG at 24 h were 1.5–2 times higher than those of [^18^F]FMISO at 3 h, with the exception of the stomach. The small tumors (80–180 mg, pO_2_ < 2.5 mmHg in 28% of tumors) were visualized in the [^18^F]FDG images but not in the [^124^I]IAZG or [^18^F]FMISO images. This may be because of the combined effect of a smaller tumor volume and a lower hypoxic fraction. The biodistribution data also showed lower uptake of the tracers in the small tumors than in the large tumors. The tumor accumulation values of [^18^F]FMISO (7.4 ± 4.4% ID/g and 11.1 ± 3.5% ID/g in large and small tumors, respectively) were higher than those of [^124^I]IAZG (1.5 ± 0.6% ID/g and 2.3 ± 0.5% ID/g in large and small tumors, respectively) at 3 h after injection. No blocking studies were performed.

Riedl et al. (13) used dynamic microPET imaging to show that [^18^F]FMISO and [^124^I]IAZG colocalized to the same intra-tumor regions in an orthotopic Morris hepatoma RH-7777 tumor model in mice. The tumor signal increased with time after [^18^F]FMISO injection, whereas the tumor signal slowly decreased after [^124^I]IAZG injection with a faster clearance from the surrounding normal tissues. The tumor/normal tissue ratios of [^124^I]IAZG increased, but they did so more slowly than those of [^18^F]FMISO in all 11 tumors in 4 mice and reached similar tumor/normal tissue ratios at a later time point (>6 h) than [^18^F]FMISO. The tumor/normal tissue ratios at 3 h for [^18^F]FMISO (1.2–2.3) were higher than those for [^124^I]IAZG (1.05–1.35). The tumor accumulation of [^18^F]FMISO (0.7 ± 0.2% ID/g) was more than two-fold higher than that of [^124^I]IAZG (0.22 ± 0.05% ID/g) at 3 h after injection. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IAZG+(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IAZG+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IAZG+human)]

No publication is currently available.

## NIH Support

CA06927, CA55893, R01 CA84596, R24 CA83084, R25 CA096945-3, P01 CA115675

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Chapman J.D., Coia L.R., Stobbe C.C., Engelhardt E.L., Fenning M.C., Schneider R.F. (1996). Prediction of tumour hypoxia and radioresistance with nuclear medicine markers. Br J Cancer Suppl.
11 Schneider R.F., Engelhardt E.L., Stobbe C.C., Fenning M.C., Chapman J.D. (1997). The synthesis and radiolabeling of novel markers of tissue hypoxia of the iodinated azomycin nucleoside class. J. Labbelled Compounds and Radiopharmaceuticals.
12 Zanzonico P., O'Donoghue J., Chapman J.D., Schneider R., Cai S., Larson S., Wen B., Chen Y., Finn R., Ruan S., Gerweck L., Humm J., Ling C. (2004). Iodine-124-labeled iodo-azomycin-galactoside imaging of tumor hypoxia in mice with serial microPET scanning. Eur J Nucl Med Mol Imaging.
13. Riedl, C.C., P. Brader, P. Zanzonico, V. Reid, Y. Woo, B. Wen, C.C. Ling, H. Hricak, Y. Fong, and J.L. Humm, Tumor hypoxia imaging in orthotopic liver tumors and peritoneal metastasis: a comparative study featuring dynamic (18)F-MISO and (124)I-IAZG PET in the same study cohort. Eur J Nucl Med Mol Imaging, 2007.